# ^64^Cu-Labeled DOTA-Lissamine Rhodamine B and derivatives

Chemical name: | ^64^Cu-Labeled Lissamine Rhodamine B and derivatives
Abbreviated name: | [^64^Cu]DOTA-LRB
Synonym:
Agent Category: | Compound
Target: | Mitochondria; P-glycoprotein transporter (P-gp)
Target Category: | Cell organelle; transporter
Method of detection: | Positron emission tomography (PET)
Source of signal / contrast: | ^64^Cu
Activation: | No
Studies: | - In vitro; - Rodents | Structure not available in PubChem (http://www.ncbi.nlm.nih.gov/pcsubstance).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=rhodamine-123&cmd=DetailsSearch)]

The mitochondrial metabolism of cancerous cells is altered to meet their high nutritional and energy demands, and this results in the production of reactive oxygen species that are believed to assist in the transformation of normal cells to the neoplastic phenotype (1). Changes in the bioenergetics of these organelles increases the negative mitochondrial potential (compared with that of mitochondria in normal cells), which can be measured with cationic organic dyes, such as rhodamine B (a fluorescent dye) and its derivatives (e.g., Lissamine rhodamine B (LRB)), because they tend to accumulate in the mitochondria (2). Therefore, several types of fluorescent tracers have been used with optical imaging techniques and have been shown to be suitable for the visualization of tumors (3, 4). In addition, ^11^C-labeled (t_1/2_ = 20.4 min) or ^18^F-labeled (t_1/2_ = 110 min) lipophilic phosphonium cation derivatives, which are rapidly taken up by the mitochondria, have also been used to detect tumors with positron emission tomography (PET) (5) and as myocardial perfusion imaging agents (6) in preclinical studies. In another study, the biodistribution of [^11^C]rhodamine-123 was investigated in mice, and it was concluded that this tracer is not suitable to measure levels of the P-glycoprotein transporter (P-gp; rhodamine dyes are known to target this transporter in the cells) (7). However, the short half-life and the generation of high background signals by this radionuclide in the normal organs of animals limits its application in the clinic (2).

In a continuing effort to develop a radiolabeled probe that would target the cellular mitochondria and would be suitable for the visualization of cancerous tumors, LRB was conjugated with 1,4,7,10-tetraazacyclododecane-1,4,7,10-tetraacetic acid (DOTA) and labeled with ^64^Cu ([^64^Cu]DOTA-LRB) (2). The main advantage of using ^64^Cu over ^11^C or ^18^F to label LRB is that the former radionuclide has a longer half-life (t_1/2_ = 12.7 h) and high specific activity. In addition, ^64^Cu is commercially available for institutions that lack an on-site cyclotron, which is required to produce ^64^Cu (2). The biodistribution of [^64^Cu]DOTA-LRB was investigated in athymic nude mice bearing U87MG cell (http://www.atcc.org/ATCCAdvancedCatalogSearch/ProductDetails/tabid/452/Default.aspx?ATCCNum=HTB-14&Template=cellBiology) glioma xenograft tumors, which express very little P-gp (2). This tracer was also evaluated for the visualization of tumors using PET (2). Yan et al. compared the biodistribution and tumor imaging properties of [^64^Cu]DOTA-LRB (designated as [^64^Cu]L1 in this study) with those of three other of ^64^Cu-labeled rhodamine derivatives (designated as [^64^Cu]L2–L4) in nude mice bearing either U87MG cell tumors or MDA-MB-435 cell tumors (these cells are known to express high levels of P-gp) (8). In addition, the use of nonradioactive [Cu]L1 was evaluated for the visualization of the U87MG cell tumors or MDA-MB-435 cell tumors in the animals.

### Related Resource Links

Optical imaging (http://www.ncbi.nlm.nih.gov/books/?term=Optical+AND+micad%5bbook%5d+AND+table%5btype%5d&view=chapter&p%24a=&p%24l=PBooksLayout&p%24st=books) chapters in MICAD

Rhodamine-related (http://www.ncbi.nlm.nih.gov/books/?term=Rhodamine+AND+micad%5bbook%5d&view=chapter&p%24a=&p%24l=PBooksLayout&p%24st=books) chapters in MICAD

Clinical trials (http://clinicaltrials.gov/ct2/results?term=Rhodamine&Search=Search) related to rhodamine

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=64Cu-DOTA-LRB%20synthesis&cmd=DetailsSearch)]

The synthesis of [^64^Cu]DOTA-LRB has been described by Zhou et al. (2). For comparison purposes, another ^64^Cu-labeled rhodamine derivative, [^64^Cu]diethylenetriamine pentaacetic acid-LRB ([^64^Cu]DTPA-LRB), was also synthesized. The radiochemical purities (RCP) of [^64^Cu]DOTA-LRB and [^64^Cu]DTPA-LRB were reported to be >95%, without high-performance liquid chromatography (HPLC) purification. The radiochemical yields (RCY) of the two tracers were not reported. The specific activities (SA) of both probes were ~1.35 TBq/mmol (~50 Ci/mmol). The final preparation of each probe was formulated in sodium chloride (pH and concentration not mentioned), and it was filtered through a 0.20-μm filter before use in animals.

In another study, Yan et al. synthesized [^64^Cu]DOTA-ethylenediamine-LRB ([^64^Cu]L1), [^64^Cu]DOTA-lysine-LRB ([^64^Cu]L2), [^64^Cu]DOTA-lysine-TAMAR-LRB ([^64^Cu]L3), and [^64^Cu]DOTA-lysine-FAM-LRB to compare their biodistribution and optical imaging properties (8). The RCYs of these radiochemicals were not reported. The RCP of each tracer was >95%, without HPLC purification; the SA of each probe was ~1.35 TBq/mmol (~50 Ci/mmol). The final preparations of the radiochemicals were formulated and filtered as described above before use in animals.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=64Cu-DOTA-LRB%20in%20vitro%20studies&cmd=DetailsSearch)]

The log P values for [^64^Cu]DOTA-LRB and [^64^Cu]DTPA-LRB were determined to be −1.4 ± 0.1 and −1.5 ± 0.1, respectively (2). [^64^Cu]DOTA-LRB was reported to be stable for >8 h after purification (storage conditions not described) (2).

For [^64^Cu]L1, [^64^Cu]L2, [^64^Cu]L3, and [^64^Cu]L4, the log P values were −1.4 ± 0.1, −1.5 ± 0.1, −1.7 ± 0.2, and −1.8 ± 0.1, respectively (8). These tracers were stable for >24 h after labeling (storage conditions not described) (8).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=64Cu-DOTA-LRB%20rodentia&cmd=DetailsSearch)]

The biodistribution of [^64^Cu]Cl_2_ was compared with that of [^64^Cu]DOTA-LRB and [^64^Cu]DTPA-LRB in athymic nude mice bearing U87MG cell tumors (2). The animals (n = 5 mice/time point for each tracer) were injected with ~0.08 MBq (~3 μCi) of the ^64^Cu-labeled tracer through the tail vein, and the rodents were euthanized at various time points ranging from 0.5 h postinjection (p.i.) to 24 h p.i. to determine the amount of radioactivity that accumulated in the various tissues. Data obtained from this study were presented as percent of injected dose per gram tissue (% ID/g). The tumor/tissue ratios derived from the uptake of radioactivity from the different probes at 4 h p.i. are shown in Table 1. The tumor/tissue ratios presented in Table 1 show that the uptake of radioactivity from [^64^Cu]Cl_2_ in the different organs was lower than that from either [^64^Cu]DOTA-LRB or [^64^Cu]DTPA-LRB. From these observations, the investigators concluded that the presence of the bifunctional metal chelators (DOTA and DTPA) within the structure of the LRB derivative had a significant influence (P value not reported) on the uptake of radioactivity from the radiotracers in the various tissues of the rodents (2). In addition, the uptake of label from [^64^Cu]DOTA-LRB in the tumors was higher than that from [^64^Cu]DTPA-LRB as demonstrated by the tumor/tissue ratios given in Table 1. No blocking studies were reported.

A mouse bearing a U87MG cell tumor was injected with ~9.25 MBq (~250 μCi) [^64^Cu]DOTA-LRB as before, and whole-body microPET images of the animal were acquired at different time points ranging from 0.5 h p.i. to 24 h p.i (2). The tumor was clearly visible in the rodent at 0.5 h p.i., and little radioactivity was detected in the brain or muscles of the animal. Data obtained with microPET imaging were similar to data from the biodistribution study (2). No blocking studies were reported.

In another study, the biodistribution of [^64^Cu]L1, [^64^Cu]L2, [^64^Cu]L3, and [^64^Cu]L4 was compared in athymic nude mice bearing U87MG cell tumors (8). The animals (n = 3–5 mice/group) were injected with ~0.08 MBq (~3 μCi) of each ^64^Cu-labeled tracer, and the rodents were euthanized at 4 h p.i. to determine the amount of radioactivity accumulated in the various organs. Data obtained from this study (Table 2) were presented as described above.

From the tumor/tissue ratios in Table 2 it is apparent that the liver had a significantly higher (P < 0.05) uptake of radioactivity from [^64^Cu]L2, [^64^Cu]L3, and [^64^Cu]L4 compared to that from [^64^Cu]L1 (8). In addition, the tumor/blood, tumor/liver, and tumor/muscle ratios with [^64^Cu]L1 were greater than those observed with the other ^64^Cu-labeled LRB tracers used in this study.

The uptake of label from [^64^Cu]L4 was also studied in MDA-MB-435 cell tumors in mice (n = 5 animals) (8). The accumulation of radioactivity in these tumors was significantly lower (1.26 ± 0.10% ID/g; P < 0.001) compared with accumulation in the U87MG cell tumors (6.25 ± 3.42% ID/g; observed in the other group of mice). The low accumulation of radioactivity in the MDA-MB-435 tumors was attributed to rapid efflux of the tracers from the lesions due to high expression of P-gp in the cells (8). No blocking studies were reported.

Mice bearing either U87Mg cell tumors or MDA-MB-435 cell tumors (n = 3 animals/tumor type) were injected with 0.5 mg nonradioactive [Cu]L1 through the tail vein for fluorescence optical imaging at 4 h p.i (8). Both types of tumors were clearly visible at 4 h p.i., and the lesions remained visible at >24 h p.i (8). No blocking studies were reported.

From these studies, the investigators concluded that ^64^Cu-labeled rhodamine derivatives can be used for the visualization of tumors with optical imaging or PET imaging techniques (8). However, more work is necessary to develop rhodamine derivatives that would show low accumulation in the liver (8).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=64Cu-DOTA-LRB%20Non-Primate%20Mammals&cmd=DetailsSearch)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=64Cu-DOTA-LRB%20Non-Human%20Primates&cmd=DetailsSearch)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=64Cu-DOTA-LRB%20Human%20Studies&cmd=DetailsSearch)]

No publication is currently available.

## Supplemental Information

[Disclaimers]

No information is currently available.

## NIH Support

This work was supported in part by grant R01 CA115883 from the National Cancer Institute, National Institutes of Health.

## References

1 Wallace D.C. (2012). Mitochondria and cancer. Nat Rev Cancer.
2 Zhou Y., et al. (2011). 64Cu-labeled lissamine rhodamine B: a promising PET radiotracer targeting tumor mitochondria. Mol Pharm.
3 Keereweer S., et al. (2012). Translational optical imaging in diagnosis and treatment of cancer. Curr Pharm Biotechnol.
4 Ebert B., Grosenick D. (2013). Optical imaging of breast tumors and of gastrointestinal cancer by laser-induced fluorescence. Recent Results Cancer Res.
5 Min J.J., et al. (2004). Tetraphenylphosphonium as a novel molecular probe for imaging tumors. J Nucl Med.
6 Shoup T.M., et al. (2011). Evaluation of (4-[18F]Fluorophenyl)triphenylphosphonium ion. A potential myocardial blood flow agent for PET. Mol Imaging Biol.
7 Bao X., et al. (2012). [(1)(1)C]Rhodamine-123: synthesis and biodistribution in rodents. Nucl Med Biol.
8 Yan X., Zhou Y., Liu S. (2012). Optical imaging of tumors with copper-labeled rhodamine derivatives by targeting mitochondria. Theranostics.

Table 1: Tumor/tissue ratios of radioactivity from [^64^Cu]Cl_2_, [^64^Cu]DOTA-LRB, and [^64^Cu]DTPA-LRB accumulated in different tissues of athymic nude mice bearing U87MG cell tumors at 4 h p.i.

Tumor/Tissue Ratios* | [^64^Cu]Cl_2_ | [^64^Cu]DOTA-LRB | [^64^Cu]DTPA-LRB
Blood | 0.39 ± 0.23 | 11.05 ± 3.87 | 2.07 ± 0.48
Heart | 0.31 ± 0.12 | 5.76 ± 3.10 | 1.66 ± 0.36
Kidney | 0.09 ± 0.02 | 1.69 ± 0.54 | 0.67 ± 0.19
Liver | 0.02 ± 0.01 | 0.96 ± 0.33 | 0.18 ± 0.03
Lungs | 0.10 ± 0.05 | 2.23 ± 0.70 | 0.99 ± 0.24
Muscle | 0.92 ± 0.34 | 29.11 ± 15.81 | 6.68 ± 1.65

*The 4-h p.i. data are presented because the accumulation of radioactivity from [^64^Cu]DOTA-LRB in the various tissues peaked at this time point (2). For complete data, see Zhou et al. (2).

Table 2: Tumor/tissue ratios of radioactivity from [^64^Cu]L1, [^64^Cu]L2, [^64^Cu]L3, and [^64^Cu]L4 accumulated in different tissues of athymic nude mice bearing U87MG cell tumors at 4 h p.i.

Tumor/Tissue Ratios | [^64^Cu]L1 | [^64^Cu]L2 | [^64^Cu]L3 | [^64^Cu]L4
Blood | 6.94 ± 0.75 | 2.00 ± 0.69 | 1.90 ± 0.66 | 4.12 ± 3.24
Liver | 0.48 ± 0.03 | 0.14 ± 0.05 | 0.15 ± 0.08 | 0.32 ± 0.17
Lungs | 1.35 ± 0.24 | 1.31 ± 0.35 | 1,35 ± 0.40 | 1.60 ± 0.52
Muscle | 35.3 ± 12.6 | 4.32 ± 1.62 | 2.25 ± 0.89 | 6.02 ± 1.88

For complete data see, Yan et al. (8).